# ^99m^Tc-Regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_

Chemical name: | ^99m^Tc-Regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_
Abbreviated name: | ^99m^Tc-RAFT-c(-RGDfK-)_4_, ^99m^Tc-RAFT-RGD
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as anti-tumor and anti-angiogenic agents, and agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced to image tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to the α_v_β_3_ integrin (50% inhibition concentration (IC_50_) = 7–40 nM) but not to the α_v_β_5_ (IC_50_ = 600–4,000 nM) or α_IIb_β_3_ (IC_50_ = 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Hydrazinonicotinic acid (HYNIC) is a coupling agent for ^99m^Tc-labeling of peptides that can achieve high specific activities without affecting the receptor-binding ability of the amino acid sequence. ^99m^Tc is bound to the hydrazine group, and other coordination sites could be occupied by one or more coligands. Liu et al. (13) reported the success of radiolabeling the cyclo(Arg-Gly-Asp-D-Phe-Lys) (c(RGDfK)) tetramer linked by glutamic acid and conjugated with HYNIC, which displayed high tumor accumulation in nude mice bearing human tumor xenografts. Boturyn et al. (14) generated a versatile molecular regioselectively addressable functionalized template (RAFT) platform with a cyclic decapeptide [c(-Lys(Boc)-Lys(Alloc)-Lys(Boc)-Pro-Gly-Lys(Boc)-Lys(Alloc)-Lys(Boc)-Pro-Gly-)] that had two attachment sides. The upper side is linked to four copies of the c(RGDfK) peptide for integrin α_v_β_3_ targeting, and the bottom side is linked to ^99m^Tc for single-photon emission computed tomography (SPECT) imaging or other labels for other imaging modalities. Sancey et al. (15) reported that ^99m^Tc-RAFT-c(-RGDfK-)_4_ efficiently accumulated into tumors in mice. ^99m^Tc-RAFT-c(-RGDfK-)_4_ is an integrin-targeted molecular imaging agent developed for imaging of tumor vasculature and tumor angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+synthesis)]

Boturyn et al. (14) described a detailed synthesis of RAFT-c(-RGDfK-)_4_ by solid-phase peptide synthesis. Radiolabeling of RAFT-c(-RGDfK-)_4_ was performed by heating 2.2–3 GBq (59–81 mCi) ^99m^Tc in a commercially available IsoLink kit at 100°C for 20 min (15). The peptide was added to one third of the mixture after neutralization with HCl; the mixture was then incubated at 60°C for 20 min. ^99m^Tc-RAFT-c(-RGDfK-)_4_ had a radiochemical purity of >95%. ^99m^Tc-RAFT-c(-RADfK-) (non-specific control) and ^99m^Tc-c(RGDfK) (specific control) were radiolabeled similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RAFT+RGD+AND%20in%20vitro)]

Boturyn et al. (14) reported that RAFT-c(-RGDfK-)_4_ inhibited CHO3a cell adhesion to vitronectin (IC_50_ = 0.5 ± 0.05 μM). RAFT-c(-RGDfK-)_4_ was internalized into the cells as observed with fluorescence microscopy. Sancey et al. (15) performed in vitro blood distribution pattern analyses of ^99m^Tc-RAFT-c(-RGDfK-)_4_ and ^9m^Tc-RAFT-c(-RADfK-) in human blood. After incubation at room temperature for 60 min, 42% and 15% of ^99m^Tc-RAFT-c(-RGDfK-)_4_ bound to globulins and cells, respectively. On the other hand, only 8% and 10% of ^99m^Tc-RAFT-c(-RADfK-) bound to globulins and cells, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+rodentia)]

Sancey et al. (15) performed biodistribution studies of ^99m^Tc-RAFT-c(-RGDfK-)_4_, ^99m^Tc-RAFT-c(-RADfK-)_4_ (non-specific control), and ^99m^Tc-c(RGDfK) (specific control) in mice bearing B16-F0 or TS/A-pc tumors. TS/A-pc tumor cells exhibited a higher level of α_v_β_3_ expression than B16-F0 tumor cells. At 60 min after injection, ^99m^Tc-RAFT-c(-RGDfK-)_4_ tumor uptake (% injected dose per gram (ID/g)) was higher than that of ^99m^Tc-c(RGDfK) and ^99m^Tc-RAFT-c(-RADfK-)_4_ in B16-F0 (2.4 ± 0.5, 1.6 ± 0.4, 1.0 ± 0.1, respectively) and in TS/A-pc tumors (2.7 ± 0.8, 1.9 ± 0.4, 0.7 ± 0.1, respectively). Liver and kidney exhibited the highest uptake. ^99m^Tc-c(RGDfK) and ^99m^Tc-RAFT-c(-RGDfK-)_4_ tumor/muscle ratios were 2.4 ± 0.5 and 3.3 ± 0.7 (P = 0.02), respectively, in B16-F0 tumors and 3.2 ± 0.8 and 2.7 ± 0.3 (P = 0.2), respectively, in TS/A-pc tumors. Planar SPECT images showed that tumor/muscle activity ratios of ^99m^Tc-c(RGDfK) and ^99m^Tc-RAFT-c(-RGDfK-)_4_ were not statistically different in mice bearing B16-F0 tumors (2.5 ± 0.8 versus 2.2 ± 0.5) and in mice bearing TS/A-pc tumors (2.8 ± 0.5 versus 2.7 ± 0.5). These ratios were significantly higher than those observed with ^99m^Tc-RAFT-c(-RADfK-)_4_ (P < 0.0002). Immunohistochemical and autoradiographic studies indicated that ^99m^Tc-RAFT-c(-RGDfK-)_4_ intratumoral uptake preferentially occurred in angiogenic areas. Quantification of transverse slices obtained from SPECT images indicated that similar tumor/muscle ratios were obtained with ^99m^Tc-c(RGDfK) and ^99m^Tc-RAFT-c(-RGDfK-)_4_ in B16-F0 tumors (2.8 ± 0.9 versus 2.3 ± 0.4) and in TS/A-pc tumors (4.1 ± 0.7 versus 4.1 ± 0.8). There was a significant difference between the ^99m^Tc-RAFT-c(-RGDfK-)_4_ tumor/muscle ratio in B16-F0 and in TS/A-pc tumors (2.3 ± 0.4 versus 4.1 ± 0.8; P < 0.01) whereas this difference did not reach statistical significance with ^99m^Tc-c(RGDfK) (2.8 ± 0.9 versus 4.1 ± 0.7; P = 0.06). The ^99m^Tc-c(RGDfK) and ^99m^Tc-RAFT-c(-RGDfK-)_4_ tumor/muscle ratios that were observed in both B16-F0 and TS/A-pc tumors were significantly higher (P < 0.05) than those obtained with ^99m^Tc-RAFT-c(-RADfK-)_4_ (1.2 ± 0.3 and 1.7 ± 0.1, respectively). No blocking study was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RAFT+RGD+AND+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Liu S., Hsieh W.Y., Jiang Y., Kim Y.S., Sreerama S.G., Chen X., Jia B., Wang F. (2007). Evaluation of a (99m)Tc-labeled cyclic RGD tetramer for noninvasive imaging integrin alpha(v)beta3-positive breast cancer. Bioconjug Chem.
14 Boturyn D., Coll J.L., Garanger E., Favrot M.C., Dumy P. (2004). Template assembled cyclopeptides as multimeric system for integrin targeting and endocytosis. J Am Chem Soc.
15 Sancey L., Ardisson V., Riou L.M., Ahmadi M., Marti-Batlle D., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2007). In vivo imaging of tumour angiogenesis in mice with the alpha(v)beta (3) integrin-targeted tracer (99m)Tc-RAFT-RGD. Eur J Nucl Med Mol Imaging.